# ^111^In-Labeled 1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid-VENK[homoC]NKEMRNRYWEAALDPNLNNQQKRAKIRSIYDDP[homoC]-NH_2_ with a disulfide bridge between the two homoC

Chemical name: | ^111^In-Labeled 1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid-VENK[homoC]NKEMRNRYWEAALDPNLNNQQKRAKIRSIYDDP[homoC]-NH_2_ with a disulfide bridge between the two homoC | [image]
Abbreviated name: | ^111^In-DOTA-MUT-DS | [image]
Synonym: | | [image]
Agent Category: | Affibody, antibody | [image]
Target: | HER2 | [image]
Target Category: | Receptor | [image]
Method of detection: | Single photon emission computed tomography (SPECT) and gamma planar imaging | [image]
Source of signal / contrast: | ^111^In | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents | Structure of ^64^Cu/^111^In-DOTA-MUT-DS by Ren et al. (1).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=affibody%20and%20HER2%20and%20molecular%20imaging)]

The ^111^In-labeled 1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid (DOTA)-VENK[homoC]NKEMRNRYWEAALDPNLNNQQKRAKIRSIYDDP[homoC]-NH_2_ (MUT-DS) conjugate with a disulfide bridge between the two homocysteines, abbreviated as ^111^In-DOTA-MUT-DS, is a 2-helix affibody derivative that was synthesized by Ren et al. for single-photon emission computed tomography (SPECT) of HER2-expressing tumors (1).

Affibody molecules are a group of nonimmunogenic scaffold proteins that are derived from the B-domain of staphylococcal surface protein A (2, 3). These molecules have only 58 amino acid residues (~7 kDa), which form a 3-α-helical bundle structure (3, 4). Helices 1 and 2 bundles are responsible for the high binding affinity and specificity of affibodies to their targets, while helix 3 contributes to the affibody stabilization and is not involved in receptor recognition (4). Studies have further confirmed that the binding domain in the helices 1 and 2 bundles includes 13 amino acid residues that are surface-exposed (2). Therefore, large affibody libraries have been constructed by randomization of the 13 amino acid residues, and a large set of affibody molecules against a wide variety of targets have been selected from those libraries. Of them, the affibodies specific to HER2, including Z_HER2:342_ and Z_HER2:477_, have been intensively investigated in recent years (3, 5). These molecules have been radiolabeled and tested for molecular imaging of HER2-expressing tumors.

The investigators at Stanford University first tested the feasibility of the monomeric (~7 kDa) and dimeric (~14 kDa) forms of affibody Z_HER2:477_ for molecular imaging (6, 7). Both forms have been labeled with various radionuclides through chelating agents. Studies have shown that smaller affibody constructs perform better in vivo in terms of tumor uptake and clearance, which prompts them to generate smaller proteins with only α-helices 1 and 2 bundles (~4 kDa) (4, 6, 7). However, simple deletion of the helix 3 leads to significantly decreased binding affinity of the proteins because of decreased helix conformation (4). The investigators then applied various strategies to improve the helix conformation of the affibody molecules, including sequence mutation, placement of disulfide bridges, and inclusion of helix-promoting amino acids (4). Although the helix conformation (~15%, the amount of α-helix represented in the secondary structure of the affibodies) of the 2-helix molecules is still much lower than that of the parent 3-helix affibodies, the investigators successfully obtained a class of 2-helix small proteins with HER2-binding affinity up to 5 nM with these strategies (1, 8, 9). One of these 2-helix proteins is MUT-DS, which has α-helices 1 and 2 bundles with a disulfide bridge being formed between the two inserted homocysteines (4). The radiolabeled MUT-DS derivatives exhibited favorable pharmacokinetics for imaging HER2-expressing tumors. ^68^Ga-DOTA-MUT-DS, ^64^Cu-DOTA-MUT-DS, ^111^In-DOTA-MUT-DS, and ^18^F-FBO-MUT-DS are examples of the MUT-DS derivatives (1, 8, 9).

This chapter summarizes the data obtained with ^111^In-DOTA-MUT-DS (1).

### Related Resource Links:

- Anti-HER2 affibody conjugates in MICAD:

^68^Ga-DOTA-Z_HER2:342-pep2_ (http://www.ncbi.nlm.nih.gov/books/NBK48901/), ^111^In-DOTA-Z_HER2:342-pep2_ (http://www.ncbi.nlm.nih.gov/books/NBK23176/), Alexa750-Z_HER2:342_ (http://www.ncbi.nlm.nih.gov/books/NBK45127/), ^111^In-benzyl-DOTA-Z_HER2:342_ (http://www.ncbi.nlm.nih.gov/books/NBK23058/), ^111^In-benzyl-DTPA-Z_HER2:342_ (http://www.ncbi.nlm.nih.gov/books/NBK23322/), Eaff800 (http://www.ncbi.nlm.nih.gov/books/NBK45665/), DY-682-ABD-Z_HER2:342_ (Haff682) (http://www.ncbi.nlm.nih.gov/books/NBK45664/), ^99m^Tc-Z_2395_-C (http://www.ncbi.nlm.nih.gov/books/NBK23590/), [^111^In]-ABY-025 (http://www.ncbi.nlm.nih.gov/books/NBK45623/), ^111^In-BZ-DTPA-Z_EGFR:1907_ (http://www.ncbi.nlm.nih.gov/books/NBK23654/).

- HER2-related clinical trials for imaging and therapy (http://clinicaltrials.gov/ct2/results?term=HER2)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/21984380)]

Ren et al. generated the cyclic 2-helix small protein DOTA-MUT-DS with standard solid-phase peptide synthesis and I_2_ oxidation of the two inserted homocysteines (1). The DOTA-MUT-DS product was purified with high-performance liquid chromatography (HPLC). The chemical yield of DOTA-MUT-DS was ~10% with >95% purity. The measured molecular weight was 5,136.77 (calculated 5,136.53).

DOTA-MUT-DS was then radiolabeled with ^111^In by reaction with ^111^InCl_3_ in NH_4_OAc buffer for 40 min at 80°C (1). After purification, the labeled ^111^In-DOTA-MUT-DS had a >95% radiochemical purity. The specific activity was 3.98–6.83 MBq/nmol (0.11–0.18 mCi/nmol) at the end of synthesis. The intact radiolabeled complex maintained >95% after 1 h incubation with mouse serum at 37°C, indicating good in vitro stability.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/21984380)]

The binding affinity with HER2 antigen and the HER2-targeting ability in cultured SKOV3 human ovarian cancer cells for DOTA-MUT-DS were measured in vitro, and the results have been presented in another report and are also summarized in the MICAD chapter of ^68^Ga-DOTA-MUT-DS (9).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/21984380)]

The biodistribution of ^111^In-DOTA-MUT-DS was examined in mice bearing SKOV3 tumors after tail vein injection of 0.26–0.3 MBq (7–8 μCi) probe (1). Mice were euthanized at 1, 4, and 20 h after injection (n = 3 mice/time point). The tumor uptake of ^111^In-DOTA-MUT-DS (2.17 ± 0.51, 3.41 ± 1.80, and 1.72 ± 0.22% injected dose per gram tissue (ID/g) at 1, 4, and 20 h after injection, respectively) was comparable to that of ^64^Cu-DOTA-MUT-DS. The blood clearance was fast, decreasing from 1.06 ± 0.13% at 1 h to 0.60 ± 0.06% and 0.18 ± 0.02% ID/g at 4 h and 20 h after injection, respectively. The tumor/blood ratios were 2.04 ± 0.39 at 1 h and 5.82 ± 2.56 at 4 h, and they reached 9.57 ± 0.93 at 20 h after injection. The tumor/muscle ratios were relatively stable, being 3.19 ± 1.45, 4.45 ± 3.16, and 3.18 ± 0.78 at 1, 4, and 20 h after injection, respectively. In normal organs, ^111^In-DOTA-MUT-DS had a higher renal accumulation than ^64^Cu-DOTA-MUT-DS, especially at later time points, being 212.00 ± 48.23%, 254.67 ± 63.55%, and 210.02 ± 31.95% ID/g at 1, 4, and 20 h after injection, respectively. The liver and intestine uptake values of ^111^In-DOTA-MUT-DS, however, were significantly lower than those of ^64^Cu-DOTA-MUT-DS at all time points (P < 0.05).

Blocking studies and PET imaging were performed with ^64^Cu-DOTA-MUT-DS, but not with ^111^In-DOTA-MUT-DS (1).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are available.

## References

1 Ren, G., J.M. Webster, Z. Liu, R. Zhang, Z. Miao, H. Liu, S.S. Gambhir, F.A. Syud, and Z. Cheng, In vivo targeting of HER2-positive tumor using 2-helix affibody molecules. Amino Acids, 2011
2 Friedman M., Nordberg E., Hoiden-Guthenberg I., Brismar H., Adams G.P., Nilsson F.Y., Carlsson J., Stahl S. (2007). Phage display selection of Affibody molecules with specific binding to the extracellular domain of the epidermal growth factor receptor. Protein Eng Des Sel.
3 Orlova A., Feldwisch J., Abrahmsen L., Tolmachev V. (2007). Update: affibody molecules for molecular imaging and therapy for cancer. Cancer Biother Radiopharm.
4 Webster J.M., Zhang R., Gambhir S.S., Cheng Z., Syud F.A. (2009). Engineered two-helix small proteins for molecular recognition. Chembiochem.
5 Gao J., Chen K., Miao Z., Ren G., Chen X., Gambhir S.S., Cheng Z. (2011). Affibody-based nanoprobes for HER2-expressing cell and tumor imaging. Biomaterials.
6 Cheng Z., De Jesus O.P., Kramer D.J., De A., Webster J.M., Gheysens O., Levi J., Namavari M., Wang S., Park J.M., Zhang R., Liu H., Lee B., Syud F.A., Gambhir S.S. (2010). 64Cu-labeled affibody molecules for imaging of HER2 expressing tumors. Mol Imaging Biol.
7 Cheng Z., De Jesus O.P., Namavari M., De A., Levi J., Webster J.M., Zhang R., Lee B., Syud F.A., Gambhir S.S. (2008). Small-animal PET imaging of human epidermal growth factor receptor type 2 expression with site-specific 18F-labeled protein scaffold molecules. J Nucl Med.
8 Miao Z., Ren G., Jiang L., Liu H., Webster J.M., Zhang R., Namavari M., Gambhir S.S., Syud F., Cheng Z. (2011). A novel (18)F-labeled two-helix scaffold protein for PET imaging of HER2-positive tumor. Eur J Nucl Med Mol Imaging.
9 Ren G., Zhang R., Liu Z., Webster J.M., Miao Z., Gambhir S.S., Syud F.A., Cheng Z. (2009). A 2-helix small protein labeled with 68Ga for PET imaging of HER2 expression. J Nucl Med.